# LTVSPWY peptide–modified PEGylated chitosan magnetic nanoparticles

Chemical name: | LTVSPWY peptide–modified PEGylated chitosan magnetic nanoparticles
Abbreviated name: | LTVSPWY-PEG-CS NPs
Synonym:
Agent Category: | Nanoparticles
Target: | Ovarian cancer cells
Target Category: | Others
Method of detection: | Optical imaging; near-infrared fluorescence (NIRF) imaging
Source of signal / contrast: | Nanoparticles
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=peptide%20as%20cancer%20drug%20delivery%20vehicles&cmd=DetailsSearch)]

Large biomolecules such as antibodies (Ab) have been extensively investigated and used for the delivery of drugs (as Ab-drug conjugates) to treat cancers, but a major limitation of using such drug delivery vehicles is that the Ab-drug conjugates are not able to penetrate deeply into solid tumors due to their large size; in addition, the conjugates may evoke an immune response, and they tend to accumulate in the liver and the reticuloendothelial system of an animal (1). Small molecules such as peptides have been shown to be efficient drug carriers, particularly if they are able to pass through the cell membrane and penetrate into the cell (such peptides are known as cell-penetrating peptides; CPP). The exact mechanism by which the CPP-drug conjugate (CPP-D) is taken up by the cells is not well understood; it is believed that the these peptides first interact with the surface and lipid components of the cell membrane, and then the CPP-D is internalized by the cell through the process of endocytosis (1). For a detailed discussion on CPPs, see Milletti (2). The heptapeptide LTVSPWY, which has a high binding specificity for human mammary adenocarcinoma SKBR3 cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-30&Template=cellBiology), was identified after the screening of several commercially available random peptide phage display libraries (3). It was shown that this peptide could be used to deliver an antisense oligonucleotide directed against the human epidermal growth factor receptor 2 (HER2, ErbB2) for internalization by the SKBR3 cells, which overexpress HER2 (3). Investigators have also reported that the LTVSPWY peptide can be used for the delivery of anticancer drugs (4, 5) and cytotoxic peptides (6) to cells under in vitro (4-6) or in vivo (5) conditions. On the basis of these studies, the biodistribution and imaging characteristics of LTVSPWY peptide–modified PEGylated chitosan magnetic nanoparticles (MNPs; LTVSPWY-PEG-CS MNPs) were studied in mice bearing SKOV-3 cell (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-77&Template=cellBiology) tumors, which overexpress HER2 (7).

### Related Resource Links

Nanoparticle related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Nanoparticles+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Nanoparticles) with nanoparticles

Clinical trials (http://clinicaltrials.gov/ct2/results?term=cell+penetrating+peptides) related to cell-penetrating peptides

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=LTVSPWY-PEG-CS%20synthesis&cmd=DetailsSearch)]

LTVSPWY-PEG-CS was synthesized as described by Jie et al. (7). Briefly, the LTVSPWY peptide was linked to poly(ethyleneglycol)2000 (PEG2000), and the complex (LTVSPWY-PEG) was conjugated to chitosan to obtain LTVSPWY-PEG-CS. The structure of LTVSPWY-PEG-CS was confirmed with proton nuclear magnetic resonance spectroscopy. PEG-CS was also prepared as described elsewhere (7).

Ferrous oxide was added to a solution of 0.1% poloxamer 188 for preparation of the MNPs as detailed by Jie et al. (7). Subsequently, a solution of LTVSPWY-PEG-CS was added to the MNP preparation, and oleic acid was added to the solution to stabilize the nanoparticles. The mixture was then sonicated and cooled to room temperature to obtain the LTVSPWY-PEG-CS MNPs. For use as controls, PEG-CS MNPs and CS MNPs were also prepared as described above. The number of LTVSPWY-PEG-CS, PEG-CS, or CS moieties conjugated on the different types of MNPs was not reported.

For imaging studies, the various MNPs were loaded with 1,1'-dioctadecyl-3,3,3',3'-tetramethyl indotricarbocyanine iodide (DiR), a near-infrared fluorescence (NIRF) dye, but the technique used to load the MNPs with the dye was not described by the investigators (7).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=LTVSPWY-PEG-CS%20in%20vitro&cmd=DetailsSearch)]

The size and zeta potential of the various magnetic NPs were as presented in Table 1.

Table 1: Size and zeta potential of the various types of MNPs ( 7 ).

Type of MNPs | Average diameter (nm)* | Zeta potential (mV)*
Unmodified | 156.0 ± 11.5 | −10.4 ± 3.5
LYVSPWY-PEG-CS modified | 267.3 ± 23.4 | 30.5 ± 7.0
PEG-CS modified | 275.0 ± 59.4 | 22.1 ± 0.8
CS modified | 278.3 ± 15.6 | 23.1 ± 1.9

*The average diameter and zeta potential of the different MNPs were determined with the dynamic light scattering technique.

Modification of the MNPs with LTVSPWY-PEG-CS, PEG-CS, or CS increased the diameter of the NPs significantly (Table 1), and the zeta potential of the particles was reversed from −10.4 ± 3.5 (unmodified MNPs) to 30.5 ± 7.0 (LTVSPWY-PEG-CS MNPs) (7). Transmission electron microscopy showed that all the MNPs had a spherical shape (7).

Cytotoxicity assays with A549 cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-185&Template=cellBiology) (a human lung carcinoma cell line that does not express HER2) and SKOV-3 cells exposed to increasing concentrations of MNPs (maximum concentration, 5 μg/mL growth medium) for up to 4 h at 37°C showed that >80% of the two cell types were viable as determined with a commercially available MTT (2H-tetrazolium,2-(4,5-dimethyl-2-thiazolyl)-3,5-diphenyl-,bromide) kit (7). This indicated that the different MNPs had low toxicity toward these cell lines.

To determine the cell-targeting specificity of the different MNPs, co-cultured SKOV-3 cells and A549 cells were exposed to LTVSPWY-PEG-CS MNPs, PEG-CS MNPs, and the CS MNPs, respectively, as described by Jie et al. (7). Fluorescence microscopy showed that the SKOV-3 cells had a higher uptake of LTVSPWY-PEG-CS MNPs compared with the A549 cells. However, both cell lines were observed to have a similar uptake of the PEG-CS MNPs and the CS MNPs, respectively. This indicated that the LTVSPWY peptide retained its cell-binding specificity even after modification with PEG-CS and conjugation to the MNPs (7). No blocking studies were reported. From this study, the investigators concluded that the CPP can be used for the cellular targeting of the MNPs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=LTVSPWY-PEG-CS%20rodentia&cmd=DetailsSearch)]

The biodistribution of DiR-loaded LTVSPWY-PEG-CS MNPs was studied in male BALB/C+nu/F1 nude mice bearing SKOV-3 cell tumors (number of animals/group or study was not reported) (7). The animals were injected with the DiR-loaded LTVSPWY-PEG-CS MNPs, PEG-CS MNPs, and CS MNPs, respectively (the net concentration of DiR in each type of MNPs was 200 μg/mL), through the tail vein (the amount of MNPs injected/animal was not reported), and whole-body NIRF images of the rodents were acquired at different time points ranging from 1 h postinjection (p.i.) to 48 h p.i. The various organs of interest were then harvested from the animals for ex vivo NIRF imaging (the time point at which the organs were harvested was not mentioned). Whole-body images acquired at 1 h p.i. showed that the fluorescence signal from the different types of MNPs was present primarily in the liver. At this time point, the tumors were visible faintly only in mice injected with the LTVSPWY-PEG-CS MNPs, and the lesions became clearly visible by 6 h p.i. for up to 48 h p.i. With PEG-CS MNPs, the tumors could be detected only at 48 h p.i., and with CS MNPs the lesions were not visible even at 48 h p.i. No blocking studies were reported.

Ex vivo images of the various organs, including the tumors, showed that with LTVSPWY-PEG-CS MNPs the intensity of the fluorescence signal (not quantified) from the liver was lower than that from the organs harvested from animals injected with either the PEG-CS MNPs or the CS MNPs (7). The intensity of the fluorescence signals of tumors obtained from the different groups was LTVSPWY-PEG-CS MNPs > PEG-CS MNPs > CS MNPs. All the MNP types were observed to accumulate in the spleen and lungs, but there was almost no uptake of the particles in the heart and the kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=LTVSPWY-PEG-CS%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=LTVSPWY-PEG-CS%20Non-Human%20Primates&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=LTVSPWY-PEG-CS%20Human%20Studies&cmd=DetailsSearch)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Zhang X.X., Eden H.S., Chen X. (2012). Peptides in cancer nanomedicine: drug carriers, targeting ligands and protease substrates. J Control Release.
2 Milletti F. (2012). Cell-penetrating peptides: classes, origin, and current landscape. Drug Discov Today.
3 Shadidi M., Sioud M. (2003). Identification of novel carrier peptides for the specific delivery of therapeutics into cancer cells. FASEB J.
4 Wang X.F., Birringer M., Dong L.F., Veprek P., Low P., Swettenham E., Stantic M., Yuan L.H., Zobalova R., Wu K., Ledvina M., Ralph S.J., Neuzil J. (2007). A peptide conjugate of vitamin E succinate targets breast cancer cells with high ErbB2 expression. Cancer Res.
5 Orban E., Manea M., Marquadt A., Banoczi Z., Csik G., Fellinger E., Bosze S., Hudecz F. (2011). A new daunomycin-peptide conjugate: synthesis, characterization and the effect on the protein expression profile of HL-60 cells in vitro. Bioconjug Chem.
6 Sioud, M. and A. Mobergslien, Selective killing of cancer cells by peptide-targeted delivery of an anti-microbial peptide. Biochem Pharmacol, 2012
7 Jie L.Y., Cai L.L., Wang L.J., Ying X.Y., Yu R.S., Zhang M.M., Du Y.Z. (2012). Actively-targeted LTVSPWY peptide-modified magnetic nanoparticles for tumor imaging. Int J Nanomedicine.